# 4-[^18^F]Fluorobenzoyl-ε-Lys^1^-c(KRGDe)MDDPGRNPHhCitGPAT

Chemical name: | 4-[^18^F]Fluorobenzoyl-ε-Lys^1^-c(KRGDe)MDDPGRNPHhCitGPAT
Abbreviated name: | [^18^F]FB-RGDechi-hCit
Synonym:
Agent category: | Peptide
Target: | α_v_β_3_ integrin
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+RGD+echistatin)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. The peptide sequence Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_ and α_v_β_5_. Various ligands have been introduced for imaging of tumors and tumor angiogenesis (8).

Various radiolabeled cyclic RGD peptides and peptidominetics have been found to have high accumulation in tumors (9, 10). Both α_v_β_3_ and α_v_β_5_ integrins bind to vitronectin (11). However, whereas the α_v_β_3_ integrin is required for basic fibroblast growth factor–mediated angiogenesis, the α_v_β_5_ integrin is required for vascular endothelial growth factor–induced angiogenesis (12, 13). Therefore, there is a need for ligands capable of discriminating between α_v_β_3_ and α_v_β_5_. Del Gatto et al. (14) have developed a series of chimeric RGD echistatin C-terminal domain (RGDechi) antagonist peptides that showed a high selectivity for the α_v_β_3_ integrin over the α_v_β_5_ integrin. One of them, c(KRGDe)MDDPGRNPHhCitGPAT (RGDechi-hCit), retains binding to α_v_β_3_ but fails to bind to α_v_β_5_. Zannetti et al. (15) used N-succinimidyl-4-[^18^F]fluorobenzoate ([^18^F]SFB) to synthesize [^18^F]FB-RGDechi-hCit for tumor targeting.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+RGD+echistatin+synthesis)]

RGDechi-hCit was prepared with solid-phase synthesis (15). [^18^F]SFB was added to a phosphate-buffered solution (pH 7.1) of 30 nmol RGDechi-hCit. The mixture was incubated for 20–60 min at room temperature. The product, [^18^F]FB-RGDechi-hCit, was purified with high-performance liquid chromatography with a specific activity of 277 MBq/nmol (7.5 mCi/nmol). The yield, radiochemical purity, and total time of synthesis were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+RGD+echistatin+in+vitro)]

Zannetti et al. (15) performed in vitro vitronectin cell adhesion assays. Transfected K562 tumor cells expressing α_v_β_3_ (Kα_v_β_3_), α_v_β_5_ (Kα_v_β_5_), or α_IIB_β_5_ (Kα_IIb_β_5_) were used in the cell adhesion assays. RGDechi (10 µM) inhibited adhesion of Kα_v_β_3_ cells to vitronectin by ~75% but did not significantly inhibit Kα_v_β_5_ and Kα_IIb_β_5_ cell adhesion to vitronectin. On the other hand, c(RGFfV) inhibited adherence to vitronectin by 60–80% in all three cells. RGDechi inhibited adhesion of U87MG cells (Kα_v_β_3_-positive and Kα_v_β_5_-negative) but had no effect on vitronectin adhesion of A431 cells (Kα_v_β_3_-negative and Kα_v_β_5_-positive). RGDechi was able to inhibit binding of ^125^I-echistatin to α_v_β_3_ but not to α_v_β_5_ and α_IIb_β_5_.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+RGD+echistatin%20rodentia)]

Zannetti et al. (15) performed ex vivo biodistribution studies of [^18^F]FB-RGDechi-hCit in nude mice bearing U87MG tumors (n = 4) or A431 tumors (n = 4) at 90 min after injection. The estimated accumulation of [^18^F]FB-RGDechi-hCit in the U87MG and A431 tumors was 0.119% injected dose per gram (ID/g) and 0.022% ID/g, respectively. The tumor/blood ratios were 3 for the U87MG tumors and 1 for the A431 tumors. The highest accumulation was found in the kidneys (0.67 and 0.47% ID/g), liver (0.17 and 0.14% ID/g), and intestine (0.17 and 0.16% ID/g) in the U87MG and A431 tumor models, respectively; accumulation in the heart and bone was not noticeable. Positron emission tomography analysis was performed after intravenous injection of 9 MBq (0.24 mCi) [^18^F]FB-RGDechi-hCit in nude mice bearing U87MG tumors in the right flank and A431 tumors in the left flank. U87MG tumors but not the A431 tumors were clearly visualized at 60 min after injection. Pretreatment with excess RGDechi-hCit prevented the accumulation of radioactivity in the U87MG tumors. Immunohistochemical staining of tumor sections confirmed the expression of α_v_β_3_ but not α_v_β_5_ in the U87MG tumors and the expression of α_v_β_5_ but not α_v_β_3_ in the A431 tumors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+RGD+echistatin+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+RGD+echistatin+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+RGD+echistatin+human)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
9 Haubner R., Decristoforo C. (2009). Radiolabelled RGD peptides and peptidomimetics for tumour targeting. Front Biosci.
10 Schottelius M., Laufer B., Kessler H., Wester H.J. (2009). Ligands for mapping alphavbeta3-integrin expression in vivo. Acc Chem Res.
11 Silva R., D'Amico G., Hodivala-Dilke K.M., Reynolds L.E. (2008). Integrins: the keys to unlocking angiogenesis. Arterioscler Thromb Vasc Biol.
12 Friedlander M., Brooks P.C., Shaffer R.W., Kincaid C.M., Varner J.A., Cheresh D.A. (1995). Definition of two angiogenic pathways by distinct alpha v integrins. Science.
13 Hood J.D., Cheresh D.A. (2002). Targeted delivery of mutant Raf kinase to neovessels causes tumor regression. Cold Spring Harb Symp Quant Biol.
14 Del Gatto A., Zaccaro L., Grieco P., Novellino E., Zannetti A., Del Vecchio S., Iommelli F., Salvatore M., Pedone C., Saviano M. (2006). Novel and selective alpha(v)beta3 receptor peptide antagonist: design, synthesis, and biological behavior. J Med Chem.
15 Zannetti A., Del Vecchio S., Iommelli F., Del Gatto A., De Luca S., Zaccaro L., Papaccioli A., Sommella J., Panico M., Speranza A., Grieco P., Novellino E., Saviano M., Pedone C., Salvatore M. (2009). Imaging of alphavbeta3 expression by a bifunctional chimeric RGD peptide not cross-reacting with alphavbeta5. Clin Cancer Res.